# Abciximab microbubbles

Chemical name: | Abciximab microbubbles
Abbreviated name: | MB_Abc_
Synonym: | Abciximab immunobubbles
Agent Category: | Antibody
Target: | Platelet glycoprotein GPIIb/IIIa
Target Category: | Antibody-antigen binding
Method of detection: | Ultrasound (US)
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=microbubbles%20AND%20abciximab)]

Ultrasound is the most widely used imaging modality (1) and its role in noninvasive molecular imaging with ligand-carrying microbubbles (MBs) is expanding (2). MBs are spherical cavities encapsulated in a shell and filled with a gas. The shells are made of phospholipids, surfactants, denatured human serum albumin, or synthetic polymers. Ligands and antibodies can be incorporated into the MB shell surface. MBs are usually 2–8 μm in diameter. MBs of this size provide a strongly reflective surface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (2-4). They may potentially be used for drug and gene delivery (5).

Abciximab (chimeric 7E3 Fab) is an FDA-approved monoclonal antibody against glycoprotein GP IIb/IIIa integrin receptor for platelet aggregation inhibition in patients undergoing percutaneous coronary intervention. Abciximab exhibited high affinity (K_d_ = 6.2 nM) for GP IIb/IIIa on platelets (6) with a B_max_ of 87,000 sites/platelet (7). MBs targeted with abciximab antibodies are being developed as noninvasive agents for ultrasonographic imaging of acute arterial thrombotic occlusion (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=microbubbles%20AND%20abciximab%20and%20synthesis)]

To produce MBs that target abciximab (MB_Abc_), Alonso et al. (8) prepared MBs by reaction of phospholipids bearing maleimido-4(p-phenylbutyrate) with thiol-activated abciximab. Control MBs (MB_c_) were also prepared using a nonspecific human Fab. The MBs were ~1.5 ± 0.2 μm in diameter with a volume diameter of 2.8 ± 0.4 μm. An antibody/MB ratio was estimated to be ~16,500 as measured by binding of ^125^I-labeled abciximab.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=microbubbles%20AND%20abciximab%20and%20in%20vitro)]

Alonso et al. (8) reported that MB_Abc_ firmly adhered to platelets in a static binding assay by microscopic examination. In contrast, negligible binding of MB_c_ was observed. Using high-resolution ultrasound imaging of blood clots in vitro, clots preincubated with specific MB_Abc_ exhibited significant contrast enhancement (37.84 ± 7.46 dB) as compared with those preincubated with nonspecific MB_c_ (28.50 ± 4.14 dB; P > 0.014) or with control clots preincubated with saline alone (20.03 ± 2.84 dB; P > 0.0006). No blocking experiment was performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=microbubbles%20abciximab%20and%20rodentia)]

Alonso et al. (8) performed ultrasound assessment of human clots in the right common carotid artery of rats. Clots pretargeted with MB_Abc_ showed a significantly higher mean grayscale value (50.09 ± 3.73) in contrast to clots preincubated with nonspecific immunobubbles (32.69 ± 6.91; P > 0.0001) and native control clots (19.56 ± 4.18; P>0.0001). Pretargeting of clots with nonspecific MB_c_ resulted in a significant increase of clot echogenicity compared with native control clots (P > 0.0037). No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=microbubbles%20abciximab%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=microbubbles%20abciximab%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=microbubbles%20abciximab%20and%20human)]

No publication is currently available.

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
5 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
6 Tam S.H., Sassoli P.M., Jordan R.E., Nakada M.T. (1998). Abciximab (ReoPro, chimeric 7E3 Fab) demonstrates equivalent affinity and functional blockade of glycoprotein IIb/IIIa and alpha(v)beta3 integrins. Circulation.
7 Wagner C.L., Mascelli M.A., Neblock D.S., Weisman H.F., Coller B.S., Jordan R.E. (1996). Analysis of GPIIb/IIIa receptor number by quantification of 7E3 binding to human platelets. Blood.
8 Alonso A., Della Martina A., Stroick M., Fatar M., Griebe M., Pochon S., Schneider M., Hennerici M., Allemann E., Meairs S. (2007). Molecular imaging of human thrombus with novel abciximab immunobubbles and ultrasound. Stroke.